# ^89^Zr-N-Succinyldesferal-anti-CD44v6 chimeric monoclonal antibody U36

Chemical name: | ^89^Zr-N-Succinyldesferal-anti-CD44v6 chimeric monoclonal antibody U36
Abbreviated name: | ^89^Zr-N-SucDf-cMAb U36, ^89^Zr-U36
Synonym:
Agent category: | Antibody, chimeric monoclonal
Target: | CD44v6
Target category: | Antigen
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^89^Zr
Activation: | No
Studies: | - In Vitro; - Rodents; - Humans | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=685122), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=48255940) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=960) for more information about CD44.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=89Zr+AND+U36)]

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (1). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (2). Invasive tumor cells adhere to the ECM, which provides a matrix environment for permeation of tumor cells through the basal lamina and underlying interstitial stroma of the connective tissue. Overexpression of matrix metalloproteinases by tumor cells allows intravasation of tumor cells into the circulatory system after degrading the basement membrane and ECM (3).

The splice variant v6 of the cell membrane glycoprotein CD44 (CD44v6) is expressed only in a few normal epithelial tissues (e.g., thyroid and prostate gland). CD44 binds to ECM and is associated with cell adhesion, lymphocyte activation, and tumor cell metastases (4, 5). Elevated levels of CD44v6 have been found in epithelial tumors, which are associated with a poor prognosis for cancer patients (5). Anti-CD44v6 chimeric (mouse/human) monoclonal antibody (cMAb) U36 was found not bind to follicles or C cells from normal human thyroid (6). CD44v6 is generally highly expressed in thyroid carcinoma (7). ^124^I-cMAb U36 was developed for imaging of CD44v6 expression in thyroid carcinoma and other epithelial tumors (8, 9). However, production of ^124^I is too expensive for routine clinical application. Verel et al. (10) explored the use of ^89^Zr positron emitter (half-life, 3.27 days) to radiolabel cMAb U36. ^89^Zr was conjugated to a bifunctional derivative of desferrioxamine B (Df) to cMAB U36 for positron emission tomography (PET) imaging of CD44v6 expression in tumors. ^89^Zr-N-Succinyldesferal-cMAb U36 (^89^Zr-N-SucDf-cMAb U36) has been studied in tumor-bearing mice and humans (11, 12).

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=CD44+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (CD44 (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=960)).
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=107269)
- Clinical trials (CD44 (http://www.clinicaltrials.gov/ct2/results?term=CD44))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=89Zr+AND+U36+synthesis)]

cMAb U36 was coupled with N-SucDf via an amide linkage and labeled with ^89^Zr (10). ^89^Zr-N-SucDf-cMAb U36 was purified with gel filtration. ^89^Zr-Labeling yields were >80%. The radiochemical purity was >97% with >90% immunoreactivity. Maximum specific activity was 83.3 MBq/nmol. There is only one lysine group per antibody molecule. ^89^Zr-N-SucDf-cMAb U36 showed no loss of ^89^Zr after incubation in human serum for 24 h at 37°C.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=89Zr+AND+U36%20and+in+vitro)]

Fortin et al. (8) reported that high-affinity ^125^I-cMAb U36 binding sites (B_max_ = 570,000 ± 30,000 sites/cell; K_d_ = 11 ± 2 nM) were found on the cell surfaces of KAT-4 human anaplastic thyroid carcinoma cells lacking the sodium iodide symporter. Furthermore, 20% of ^125^I-cMAb U36 accumulated in the cells after incubation for 24 h at 37°C. Accumulation was reduced to 1% with excess cMAb U36. The labeled cells retained 29% of the radioactivity after incubation in tracer-free medium alone for another 24 h at 37°C.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=89Zr+AND+U36%20and+rodentia)]

Verel et al. (10) performed ex vivo biodistribution studies and in vivo PET imaging studies of ^89^Zr-N-SucDf-cMAb U36 in nude mice (n = 4/group) bearing HNX-OE human head and neck tumors at 24, 48, and 72 h after injection. ^89^Zr-N-SucDf-cMAb U36 uptake in the tumors was 14.1 ± 1.0%, 22.0 ± 2.0%, and 26.0 ± 1.9% injected dose per gram (ID/g) at 24, 48, and 72 h, respectively. The blood level of ^89^Zr-N-SucDf-cMAb U36 decreased from 14.6% at 24 h to 12.3% ID/g at 72 h. Most nontarget organs exhibited ~5% ID/g. Selective tumor uptake was confirmed with PET imaging at 24, 48, and 72 h, detecting 12 of 12 tumors (as small as 19 mg). Only the blood pool in the heart and liver was visible. The results of these studies were similar to those reported for ^124^I-cMAb U36 in the same tumor model (9). No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=89Zr+AND+U36%20and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=89Zr+AND+U36%20and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=89Zr+AND+U36%20and+human)]

Borjesson et al. (11) performed PET imaging with 75 MBq (2 mCi) ^89^Zr-N-SucDf-cMAb U36 in 20 cancer patients with head and neck squamous cell carcinoma (HNSCC) at 1, 24, 72, and 144 h after injection. All primary tumors, lymph node metastases in 18 of 25 positive levels (sensitivity 72%) and in 11 of 15 positive sides (sensitivity 73%) were observed. Interpretation of the PET data was correct in 112 of 121 operated levels with 93% accuracy and in 19 of 25 operated sides with 76% accuracy. For CT/MRI, sensitivities of 60% and 73% and accuracies of 90% and 80% were observed per level and side, respectively. In the six patients with seven tumor-involved neck levels and sides, ^89^Zr-N-SucDf-cMAb U36 PET and [^18^F]fluoro-2-deoxy-D-glucose PET yielded comparable diagnostic results.

Borjesson et al. (12) performed radiation dosimetry of ^89^Zr-N-SucDf-cMAb U36 in 20 cancer patients with HNSCC. PET scans were performed at 1, 24, 72, and 144 h after injection of 75 MBq (2.0 mCi) ^89^Zr-N-SucDf-cMAb U36. For men, the highest absorbed doses were in the liver (1.25 ± 0.27 mSv/MBq), thyroid (0.91 ± 0.27 mSv/MBq), kidneys (0.82 ± 0.15 mSv//MBq), spleen (0.67 ± 0.11 mSv//MBq), and lungs (0.63 ± 0.20 mSv//MBq). The effective dose was 0.53 ± 0.03 mSv/MBq. For women, the absorbed doses in these organs were ~10–20% higher than those for men with an effective dose of 0.66 ± 0.03 mSv/MBq. ^89^Zr-N-SucDf-cMAb U36 accumulation in tumors increased over time, whereas accumulation in most organs decreased over time. The mean tumor accumulation was 0.019 ± 0.010% ID/g at 168 h after injection as assessed with biopsies.

## References

1 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
2 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
3 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
4 Van Hal N.L., Van Dongen G.A., Rood-Knippels E.M., Van Der Valk P., Snow G.B., Brakenhoff R.H. (1996). Monoclonal antibody U36, a suitable candidate for clinical immunotherapy of squamous-cell carcinoma, recognizes a CD44 isoform. Int J Cancer.
5 Heider K.H., Kuthan H., Stehle G., Munzert G. (2004). CD44v6: a target for antibody-based cancer therapy. Cancer Immunol Immunother.
6 Schrijvers A.H., Quak J.J., Uyterlinde A.M., van Walsum M., Meijer C.J., Snow G.B., van Dongen G.A. (1993). MAb U36, a novel monoclonal antibody successful in immunotargeting of squamous cell carcinoma of the head and neck. Cancer Res.
7 Aogi K., Kitahara K., Urquidi V., Tarin D., Goodison S. (1999). Comparison of telomerase and CD44 expression as diagnostic tumor markers in lesions of the thyroid. Clin Cancer Res.
8 Fortin M.A., Salnikov A.V., Nestor M., Heldin N.E., Rubin K., Lundqvist H. (2007). Immuno-PET of undifferentiated thyroid carcinoma with radioiodine-labelled antibody cMAb U36: application to antibody tumour uptake studies. Eur J Nucl Med Mol Imaging.
9 Verel I., Visser G.W., Vosjan M.J., Finn R., Boellaard R., van Dongen G.A. (2004). High-quality 124I-labelled monoclonal antibodies for use as PET scouting agents prior to 131I-radioimmunotherapy. Eur J Nucl Med Mol Imaging.
10 Verel I., Visser G.W., Boellaard R., Stigter-van Walsum M., Snow G.B., van Dongen G.A. (2003). 89Zr immuno-PET: comprehensive procedures for the production of 89Zr-labeled monoclonal antibodies. J Nucl Med.
11 Borjesson P.K., Jauw Y.W., Boellaard R., de Bree R., Comans E.F., Roos J.C., Castelijns J.A., Vosjan M.J., Kummer J.A., Leemans C.R., Lammertsma A.A., van Dongen G.A. (2006). Performance of immuno-positron emission tomography with zirconium-89-labeled chimeric monoclonal antibody U36 in the detection of lymph node metastases in head and neck cancer patients. Clin Cancer Res.
12 Borjesson P.K., Jauw Y.W., de Bree R., Roos J.C., Castelijns J.A., Leemans C.R., van Dongen G.A., Boellaard R. (2009). Radiation dosimetry of 89Zr-labeled chimeric monoclonal antibody U36 as used for immuno-PET in head and neck cancer patients. J Nucl Med.